# 6-[^18^F]Fluoro-3-[2(S)-2-azetidinylmethoxy]pyridine

Chemical name: | 6-[^18^F]Fluoro-3-[2(S)-2-azetidinylmethoxy]pyridine
Abbreviated name: | 6-[^18^F]FA
Synonym: | 6-[^18^F]Fluoro-A-85380
Agent Category: | Compound
Target: | α4β2 nicotinic acetylcholine receptor (nAChR)
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-18F%20A-85380)]

Neuronal nicotinic cholinergic receptors (nAChRs) are a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine always causes a rapid increase in cellular permeability to ions, such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α (α2-α10) and four subtypes of structural β (β2-β5). nAChRs have been demonstrated to be involved in cognitive processes such as learning and memory and control of movement in normal subjects. Dysfunction of nAChR has been implicated to a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease (AD) and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and related health problems associated with tobacco smoking.

3-[2(S)-2-azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4, 5). A-85380 has been labeled as 6-[^18^F]Fluoro-3-[2(S)-2-azetidinylmethoxy]pyridine (6-[^18^F]fluoro-A-85380) (6-8). 6-[^18^F]fluoro-A-85380 (6-[^18^F]FA) is being developed as a PET agent for the non-invasive study of nAChR in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-18F%20A-85380%20and%20synthesis)]

Scheffel et al. (7) reported synthesis of 6-[^18^F]FA by a 2-step reaction, which consisted of standard ([^18^F]KF/Kryptofix 2.2.2) ^18^F-nucleophilic aromatic fluorination of 6-iodo-3-[2-((S)-N-tert-butoxycarbonyl-3-pyrroline)methoxy]pyridine and acidic deprotection of the product. An average radiochemical yield was 15% (end of synthesis, based on [^18^F]KF, not corrected for decay) with a total synthesis time of 83-98 min. The average specific activity was 96 GBq/μmol (2.6 Ci/μmol) at end of synthesis with a radiochemical purity of >99%. Horti et al. (8) reported a similar synthesis of 6-[^18^F]FA with a radiochemical yield of up to 21% (not corrected for decay) and specific activities of 100-200 GBq/μmol (1.2-5.4 Ci/μmol). Ding et al. (6) reported an improved synthesis of 6-[^18^F]FA with 38-48% yield (end of bombardment) in 50-55 min using 6-trimethylammonium-3-[2-((S)-N-tert-butoxycarbonyl-3-pyrroline)methoxy]pyridine with specific activity of 74-185 GBq/μmol (2-5 Ci/μmol) at end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-18F%20A-85380%20and%20in%20vitro)]

Sullivan et al. (4) reported that A-85380 had K_i_ values of 0.05 ± 0.01, 148 ± 13, and 314 ± 12 nM for human α4β2, α7, and muscle α1β1δγ receptors, respectively. A-85380 (up to 10,000 nM) has no effect in various neurotransmitter binding assays. Gundisch et al. (9) reported that 6-FA had K_i_ values of 0.026 ± 0.004, 14 ± 2, 170± 10, and 460 ± 50 nM for rat α4β2, α3β4, α7, and muscle α1β1δγ receptors, respectively. Epibatidine, 6-FA, cytisine and nictotine had K_i_ values (obtained by use of 6-[^18^F]FA) of 11, 25, 120, and 870 pM for α4β2, respectively. Horti et al. (8) determined that 6-[^18^F]FA had a K_d_ of 28 ± 2 pM and a B_max_ of 153 ± 17 fmol/mg protein in rat brain homogenates. Gundisch et al. (9) reported that 6-[^18^F]FA had a K_d_ of 26 ± 1 pM and a B_max_ of 760 ± 0.15 fmol/g tissue in postmortem human cortical membranes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-18F%20A-85380%20and%20rodentia)]

Scheffel et al. (7) performed biodistribution studies in mouse brain after injection of 0.74 MBq (20 μCi) 6-[^18^F]FA (0.3 nmol/kg). A peak uptake of 1.92% injected dose (ID)/g was reached in the whole brain at 15 min, followed by a gradual washout. 6-[^18^F]FA accumulation was peaked in the thalamus (8.2% ID/g) and in superior colliculus (7.5% ID/g) at 60 min and lower in the hippocampus (3.5% ID/g) and cerebellum (3.5% ID/g), which peaked at 15 min post injection and had more rapid washout than the thalamus and superior colliculus. Nicotine, cytosine or 6-FA administered before or after 6-[^18^F]FA injection significantly inhibited binding in all regions of the brain including the cerebellum. Scopolamine (a muscarinic AChR antagonist) and mecamylamine (a nAChR channel blocker) did not exhibit any inhibition. Pretreatment with 6-FA (125 nmol/kg) blocked accumulation in the thalamus by 87%. No signs of toxicity were observed in the mice in these experiments.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-18F%20A-85380%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit%20or%20cat))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-18F%20A-85380%20and%20(primate%20not%20human))]

Ding et al. (6) compared 6-[^18^F]FA and 2-[^18^F]FA in PET studies with one baboon showing substantial brain accumulation with selective maximal uptake of both tracers in the regions of the thalamus (0.017% ID/cc), striatum (0.014% ID/cc) and cerebellum (0.014% ID/cc). However, 6-[^18^F]FA peaked earlier than 2-[^18^F]FA. Cerebellum cleared 6-[^18^F]FA faster (t_1/2_ = 120 min) than 2-[^18^F]FA (t_1/2_ = 190 min). Thalamus-to-cerebellum distribution volume ratio was higher for 6-[^18^F]FA (2.5-3.5) than 2-[^18^F]FA (1.9-2.1) at 180 min. Therefore, 6-[^18^F]FA exhibited a faster kinetics than 2-[^18^F]FA. The fraction of unchanged 6-[^18^F]FA in the plasma was 26% at 30 min versus 52% with 2-[^18^F]FA.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-18F%20A-85380%20and%20(human%20not%20human%5bText%20Word%5d))]

In a PET study of α4β2 nAChR distribution in human brain (five healthy nonsmokers), Ding et al. (10) reported that 6-[^18^F]FA showed major localization of radioactivity in the thalamus, brain stem and putamen. Distribution volume ratios and binding potentials (BPs) were calculated using a one-compartment model with corpus callosum as a reference tissue. The thalamus had a BP of 3.1. Equilibrium was achieved at 50-60 min after injection. Total scanning time was 2 h for sufficient and reproducible kinetic analysis. The fraction of unchanged 6-[^18^F]FA in plasma was 50% at 60 min.

## NIH Support

Intramural Research Program

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
5 Abreo M.A., Lin N.H., Garvey D.S., Gunn D.E., Hettinger A.M., Wasicak J.T., Pavlik P.A., Martin Y.C., Donnelly-roberts D.L., Anderson D.J., Sullivan J.P., Williams M., Arneric S.P., Holladay M.W. (1996). Novel 3-Pyridyl ethers with subnanomolar affinity for central neuronal nicotinic acetylcholine receptors. J Med Chem.
6 Ding Y., Liu N., Wang T., Marecek J., Garza V., Ojima I., Fowler J.S. (2000). Synthesis and evaluation of 6-[(18)F]fluoro-3-(2(S)-azetidinylmethoxy)pyridine as a PET tracer for nicotinic acetylcholine receptors. Nucl Med Biol.
7 Scheffel U., Horti A.G., Koren A.O., Ravert H.T., Banta J.P., Finley P.A., London E.D., Dannals R.F. (2000). 6-[18F]Fluoro-A-85380: an in vivo tracer for the nicotinic acetylcholine receptor. Nucl Med Biol.
8 Horti A.G., Chefer S.I., Mukhin A.G., Koren A.O., Gundisch D., Links J.M., Kurian V., Dannals R.F., London E.D. (2000). 6-[18F]fluoro-A-85380, a novel radioligand for in vivo imaging of central nicotinic acetylcholine receptors. Life Sci.
9 Gundisch D., Koren A.O., Horti A.G., Pavlova O.A., Kimes A.S., Mukhin A.G., London E.D. (2005). In vitro characterization of 6-[18F]fluoro-A-85380, a high-affinity ligand for alpha4beta2* nicotinic acetylcholine receptors. Synapse.
10 Ding Y.S., Fowler J.S., Logan J., Wang G.J., Telang F., Garza V., Biegon A., Pareto D., Rooney W., Shea C., Alexoff D., Volkow N.D., Vocci F. (2004). 6-[18F]Fluoro-A-85380, a new PET tracer for the nicotinic acetylcholine receptor: studies in the human brain and in vivo demonstration of specific binding in white matter. Synapse.